# Biotinylated anti-Tn MLS128 monoclonal antibody-streptavidin-^111^In-DTPA-biotin

Chemical name: | Biotinylated anti-Tn MLS128 monoclonal antibody-streptavidin-^111^In-DTPA-biotin
Abbreviated name: | Bt-MLS128-SA-^111^In-biotin
Synonym:
Agent Category: | Antibody
Target: | Tumor-associated carbohydrate Tn antigen
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=%22Tn%20antigen%22)]

Tn antigen is a tumor-associated carbohydrate epitope (N-acetyl-galactosamine (GalNAc)-O-Ser/Thr (GalNAca-O-Ser/Thr)) (1-3). Three-step targeting with biotinylated MLS128 monoclonal antibody (Bt-MLS128 mAb), streptavidin (SA), and ^111^In-diethylenetriamine pentaacetic acid (DTPA)-biotin (^111^In-biotin) was developed for in vivo imaging of Tn antigen-expressing tumors (4). It was designed on the basis of avidin’s extraordinarily high binding affinity for biotin.

Avidin’s high affinity for biotin was first exploited in histochemical applications in the mid-1970s (5, 6). This affinity is more than one million times higher than that of most antibodies for most antigens. Avidin has four binding sites for biotin, and most proteins, including enzymes, can be conjugated with several molecules of biotin. The avidin-biotin binding is essentially irreversible. These properties allow molecular complexes to be formed between avidin and biotinylated antibodies. In addition, small molecular sizes of avidin and biotin allow improved tumor uptake and rapid intratumoral spatial distribution.

Altered glycosylation on the cell surface is a hallmark of malignant transformation and tumor progression. Incomplete synthesis of the carbohydrate chains and precursor accumulation result in loss of the normal carbohydrate antigens and high expression of the tumor-associated carbohydrate antigens (7-9). Lewis Y, TF, Globo H, GM2, polysialic acid, sialyl Lewis A, Tn, and sialyl Tn are some of the antigens investigated intensively as diagnostic markers or as vaccine antigens (8-11). Tn antigen was first reported as a tumor-associated antigen nearly 40 years ago (12). It is composed of a single GalNAc glycan residue attached via an α-linkage to either the serine (Ser) or the threonine (Thr) of a polypeptide chain (9, 11). In normal tissues, Tn antigen is masked by covalently bound terminal carbohydrate moieties, but in tumors it is unmasked because of defective O-glycosylation. Accordingly, Tn antigen is rarely expressed in normal tissues, but it is widely expressed in human carcinomas or hematological cancers. It has been reported that the Tn antigen is expressed in 70–90% of breast, colon, lung, bladder, cervical, ovarian, stomach, and prostate tumors (1, 3, 7). The expression levels of the Tn antigen are closely associated with tumor aggressiveness and poor survival of patients (8, 10). In addition, Tn antigen is recognized by the human immune system as a novel epitope, provoking immune responses in patients. There is a strong correlation among the expression of the Tn antigen, the development of the spontaneous antibodies against Tn, and the prognosis for patients with carcinomas. Clinical trials are under way to deliberately provoke or enhance human immune responses by injecting patients with synthetic peptide antigens bearing Tn structure (3, 8, 13-15). Tn antigen has attracted significant interest as a target for tumor diagnosis and immunotherapy. A number of anti-Tn IgG and IgM antibodies have been generated and investigated for their imaging feasibilities and anti-tumor activities (2, 4, 16-22). The results are generally inconsistent. There are still some issues to be resolved, such as immunogenicity, reduced effectiveness in vivo, and cross-reactivity against type-A blood antigen. In addition, directly radiolabeled antibodies usually show a slow and low uptake by tumors, and their blood clearance is also slow. Nakamoto et al. tested the imaging feasibility of three-step targeting with Bt-MLS128, SA, and ^111^In-biotin in mice bearing LS180 human colon cancer xenografts (4).

Note: Investigators from the same research group as Nakamoto et al. also labeled the anti-Tn MLS128 mAb directly with ^125^I/^131^I (^125^I/^131^I-MLS128 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) and ^111^In (^111^In-MLS128 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)), separately, and investigated their biodistribution and the feasibility of imaging tumors in mice bearing LS180 tumor xenografts. They also tested the imaging feasibility of two-step targeting with Bt-MLS128 and ^125^I-SA (Bt-MLS128-^125^I-SA (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) in mice with LS180 tumor xenografts (17, 19, 20, 23, 24).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Imaging with three-step targeting included three agents: Bt-MLS128, SA, and ^111^In-biotin (4, 20). The anti-Tn MLS128 is a mouse IgG3 antibody with κ light chain, and it was produced by immunizing mice with LS180 human colorectal cancer cells (21). The antibody was purified from the ascitic fluid of the hybridoma-bearing mice with protein A affinity chromatography. The murine OST6 mAb against an alkaline phosphatase-related substance was used as the control. The antibodies were biotinylated by mixing them with sulfosuccinimidyl-6-(biotinamido)hexanoate, and they were then purified with chromatography on PD-10 gel. The average numbers of biotin molecules coupled to the MLS128 and OST6 were 1.2 and 1.7, respectively. Bt-MLS128, Bt-OST6, and SA were also labeled with ^125^I with the chloramine-T method. The labeling efficiencies of radioiodinated Bt-MLS128, Bt-OST6, and SA were 63.2, 58.3, and 81.3%, respectively, and their specific activities were 23.4, 21.6, and 30.1 GBq/µg (0.63, 0.58, and 0.81 kCi/µg), respectively. The ^111^In-DTPA-biotin was developed by mixing DTPA-biotin with ^111^In-chloride. The labeling efficiency of the ^111^In-biotin was >99%, and its specific activity was 296.0 GBq/µg (8 kCi/µg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Nakamoto et al. analyzed the binding abilities of ^125^I-Bt-MLS128 and ^125^I-SA to the immobilized avidin, biotin, and LS180 tumor cells by incubating them together for 1 h at 4ºC (4). More than 95% of ^125^I-Bt-MLS128 bound to immobilized avidin. The immunoreactive fraction of ^125^I-Bt-MLS128 that bound to the LS180 tumor cells was 47.2%, which was slightly lower than that of the unmodified MLS128 (data not shown). ^125^I-SA showed >90% binding to the biotin-coated beads. There was no significant binding between the control ^125^I-Bt-OST6 and the LS180 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Nakamoto et al. analyzed the biodistribution of the Bt-MLS128, ^125^I-SA, and ^111^In-biotin system in female BALB/c nu/nu mice bearing subcutaneous LS180 tumor xenografts (4). The mice were pretreated with intravenous (i.v.) administration of Bt-MLS128, followed by i.v. injection of ^125^I-SA 2 days later. ^111^In-biotin was administered via i.v. injection on day 1, 4, or 7, separately, after injection of ^125^I-SA (n = 4–5 mice/time point). The mice were euthanized 2 h later, and the radioactivity levels of ^125^I and ^111^In were simultaneously counted with dual-channel counting. For the control mice, Bt-OST6 was given to the mice instead of Bt-MLS128.

The biodistribution data collected by counting the ^125^I-SA accumulation showed that the tumor had a significantly higher uptake of ^125^I-SA in the Bt-MLS128–pretreated mice than in control mice (P < 0.05). The ^125^I-SA radioactivity in the tumors decreased gradually over time: 6.39 ± 1.23, 4.66 ± 0.52, and 3.24 ± 0.92% injected dose per gram of tissue (ID/g) on days 1, 4, and 7, respectively. The radioactivity levels of ^125^I-SA decreased much faster in blood than in tumors: 1.75 ± 0.32, 0.5 ± 0.17, and 0.28 ± 0.03% ID/g in blood on days 1, 4, and 7, respectively. The difference in ^125^I-SA clearance between the tumor and blood resulted in increased tumor/blood ratios over time: 3.69, 9.90, and 11.62, on days 1, 4, and 7, respectively (P < 0.05). Among the organs examined, the kidney had the highest level of ^125^I-SA radioactivity: 44.67 ± 6.58, 44.04 ± 7.12, and 26.36 ± 2.08% ID/g on days 1, 4, and 7, respectively. The biodistribution data collected by counting the ^111^In-biotin accumulation also showed that the tumor had a significantly higher level of ^111^In-biotin radioactivity in the Bt-MLS128–pretreated mice than in control mice (0.51 ± 0.07 versus 0.14 ± 0.01% ID/g on day 4, P < 0.05). The radioactivity levels of ^111^In-biotin in the tumors decreased with the prolonged interval between injections of ^125^I-SA and ^111^In-biotin, but the facilitated blood clearance of ^111^In-biotin compensated for the decreased tumor uptake, providing higher tumor/blood ratios. The radioactivity levels in the tumors were 1.41 ± 0.24, 0.51 ± 0.07, and 0.56 ± 0.14% ID/g, respectively, and the tumor/blood ratios were 1.51, 2.61, and 4.01, on day 1, 4, or 7, respectively (P < 0.05). Again, among the organs examined, the kidney had the highest level of ^111^In-biotin radioactivity: 8.83 ± 1.81, 6.97 ± 0.70, and 5.88 ± 1.29% ID/g on days 1, 4, and 7, respectively. Scintigraphic images were consistent with the results of biodistribution data. Clear tumor images were obtained as early as 2 h after injection of ^111^In-biotin.

Zhang et al. from the same research group as Nakamoto et al. analyzed the biodistribution of the Bt-MLS128, SA, and ^111^In-biotin system in female BALB/c nu/nu mice bearing LS180 intraperitoneal tumor xenografts (20). The study involved i.v. pretreatment with Bt-MLS128 for 48 h, followed by intraperitoneal (i.p.) injection of SA. At 24 h after SA injection, ^111^In-biotin was administered via i.v. or i.p. injection, and the mice were euthanized 2 h later. The data showed that i.p. injection of ^111^In-biotin resulted in significantly higher tumor uptake (9.54 ± 3.51 versus 3.60 ± 0.77% ID/g, P < 0.05) and tumor/blood ratio (2.80 ± 1.24 versus 1.03 ± 0.21, P < 0.05) than i.v. injection. With increasing doses from 0.3 µg to 10 µg of ^111^In-biotin, the tumor uptake of ^111^In-biotin decreased (9.54 ± 3.51 versus 1.47 ± 0.30% ID/g, P = 0.007), but the tumor/blood ratio was not different (2.80 ± 1.24 versus 2.97 ± 0.44, P > 0.5). It is worth noting that the relative doses of the various reagents in multistep targeting are more complicated than that of antibody in one-step targeting. Tumor uptake of the ^125^I-SA improved with an increased dose of Bt-MLS128. However, this also provided more antibodies in circulation and slowed down the clearance of radioactivity, thus affecting the tumor/blood ratio. On the other hand, the higher dose of radiolabeled SA or biotin decreased the tumor uptake of radioactivity, which may be related to relative limited number of the binding site in tumor. At the same time, the less complex formed in circulation, the faster the clearance of radioactivity, leading to less change of the tumor/blood ratio.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Springer G.F. (1997). Immunoreactive T and Tn epitopes in cancer diagnosis, prognosis, and immunotherapy. J Mol Med.
2 Ando H., Matsushita T., Wakitani M., Sato T., Kodama-Nishida S., Shibata K., Shitara K., Ohta S. (2008). Mouse-human chimeric anti-Tn IgG1 induced anti-tumor activity against Jurkat cells in vitro and in vivo. Biol Pharm Bull.
3 Li Q., Anver M.R., Butcher D.O., Gildersleeve J.C. (2009). Resolving conflicting data on expression of the Tn antigen and implications for clinical trials with cancer vaccines. Mol Cancer Ther.
4 Nakamoto Y., Saga T., Sakahara H., Yao Z., Zhang M., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Three-step tumor imaging with biotinylated monoclonal antibody, streptavidin and 111In-DTPA-biotin. Nucl Med Biol.
5 Becker J.M., Wilchek M. (1972). Inactivation by avidin of biotin-modified bacteriophage. Biochim Biophys Acta.
6 Hsu S.M., Raine L., Fanger H. (1981). Use of avidin-biotin-peroxidase complex (ABC) in immunoperoxidase techniques: a comparison between ABC and unlabeled antibody (PAP) procedures. J Histochem Cytochem.
7 Babino A., Oppezzo P., Bianco S., Barrios E., Berois N., Navarrete H., Osinaga E. (2000). Tn antigen is a pre-cancerous biomarker in breast tissue and serum in n-nitrosomethylurea-induced rat mammary carcinogenesis. Int J Cancer.
8 Hakomori S. (2001). Tumor-associated carbohydrate antigens defining tumor malignancy: basis for development of anti-cancer vaccines. Adv Exp Med Biol.
9 Kulkarni K.A., Sinha S., Katiyar S., Surolia A., Vijayan M., Suguna K. (2005). Structural basis for the specificity of basic winged bean lectin for the Tn-antigen: a crystallographic, thermodynamic and modelling study. FEBS Lett.
10 Kurtenkov O., Klaamas K., Rittenhouse-Olson K., Vahter L., Sergejev B., Miljukhina L., Shljapnikova L. (2005). IgG immune response to tumor-associated carbohydrate antigens (TF, Tn, alphaGal) in patients with breast cancer: impact of neoadjuvant chemotherapy and relation to the survival. Exp Oncol.
11 Lescar J., Sanchez J.F., Audfray A., Coll J.L., Breton C., Mitchell E.P., Imberty A. (2007). Structural basis for recognition of breast and colon cancer epitopes Tn antigen and Forssman disaccharide by Helix pomatia lectin. Glycobiology.
12 Dausset J., Moullec J., Bernard J. (1959). Acquired hemolytic anemia with polyagglutinability of red blood cells due to a new factor present in normal human serum (Anti-Tn). Blood.
13 Springer G.F., Desai P.R., Spencer B.D., Tegtmeyer H., Carlstedt S.C., Scanlon E.F. (1995). T/Tn antigen vaccine is effective and safe in preventing recurrence of advanced breast carcinoma. Cancer Detect Prev.
14 Slovin S.F., Ragupathi G., Musselli C., Olkiewicz K., Verbel D., Kuduk S.D., Schwarz J.B., Sames D., Danishefsky S., Livingston P.O., Scher H.I. (2003). Fully synthetic carbohydrate-based vaccines in biochemically relapsed prostate cancer: clinical trial results with alpha-N-acetylgalactosamine-O-serine/threonine conjugate vaccine. J Clin Oncol.
15 Cipolla L., Rescigno M., Leone A., Peri F., La Ferla B., Nicotra F. (2002). Novel Tn antigen-containing neoglycopeptides: synthesis and evaluation as anti tumor vaccines. Bioorg Med Chem.
16 Takahashi H.K., Metoki R., Hakomori S. (1988). Immunoglobulin G3 monoclonal antibody directed to Tn antigen (tumor-associated alpha-N-acetylgalactosaminyl epitope) that does not cross-react with blood group A antigen. Cancer Res.
17 Yao Z., Sakahara H., Zhang M., Kobayashi H., Nakada H., Yamashina I., Konishi J. (1995). Radioimmunoimaging of colon cancer xenografts with anti-Tn monoclonal antibody. Nucl Med Biol.
18 Yao Z., Zhang M., Sakahara H., Saga T., Kobayashi H., Nakamoto Y., Toyama S., Konishi J. (1998). Increased streptavidin uptake in tumors pretargeted with biotinylated antibody using a conjugate of streptavidin-fab fragment. Nucl Med Biol.
19 Zhang M., Yao Z., Saga T., Sakahara H., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1998). Improved intratumoral penetration of radiolabeled streptavidin in intraperitoneal tumors pretargeted with biotinylated antibody. J Nucl Med.
20 Zhang M., Yao Z., Sakahara H., Saga T., Nakamoto Y., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Effect of administration route and dose of streptavidin or biotin on the tumor uptake of radioactivity in intraperitoneal tumor with multistep targeting. Nucl Med Biol.
21 Numata Y., Nakada H., Fukui S., Kitagawa H., Ozaki K., Inoue M., Kawasaki T., Funakoshi I., Yamashina I. (1990). A monoclonal antibody directed to Tn antigen. Biochem Biophys Res Commun.
22 Oppezzo P., Osinaga E., Tello D., Bay S., Cantacuzene D., Irigoin F., Ferreira A., Roseto A., Cayota A., Alzari P., Pritsch O. (2000). Production and functional characterization of two mouse/human chimeric antibodies with specificity for the tumor-associated Tn-antigen. Hybridoma.
23 Yao Z., Zhang M., Kobayashi H., Sakahara H., Nakada H., Yamashina I., Konishi J. (1995). Improved targeting of radiolabeled streptavidin in tumors pretargeted with biotinylated monoclonal antibodies through an avidin chase. J Nucl Med.
24 Zhang M., Sakahara H., Yao Z., Saga T., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1997). Intravenous avidin chase improved localization of radiolabeled streptavidin in intraperitoneal xenograft pretargeted with biotinylated antibody. Nucl Med Biol.